# ^99m^Tc-Labeled O-[3-(1,4,8,11-tetraazabicyclohexadecane)-propyl]-α-methyl tyrosine

Chemical name: | ^99m^Tc-Labeled O-[3-(1,4,8,11-tetraazabicyclohexadecane)-propyl]-α-methyl tyrosine
Abbreviated name: | [^99m^Tc]-N4-AMT
Synonym:
Agent Category: | Compound
Target: | L-type amino acid transporter
Target Category: | Transporter
Method of detection: | Single-photon emission computed tomography (SPECT); gamma planar imaging
Source of signal / contrast: | ^99m^Tc
Activation: | No
Studies: | - In vitro; - Rodents | Click on above structure of N4-AMT for information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=amino%20acid%20and%20imaging%20and%20amino%20acid%20transporters)]

High energy consumption and rapid proliferation are the distinct characteristics of all cells with a malignant phenotype. To maintain a high pace of protein and DNA synthesis, such cells have an increased demand for various nutrients, glucose, and amino acids (aa). Therefore, radiotracers such as ^18^F-labeled fluorodeoxyglucose, which is taken up by the cell through the glucose transporter, are often used with positron emission tomography to detect cancerous tumors. This agent, however, is not suitable to distinguish between malignant tissue, inflammation, and tissues that normally have high glucose consumption, such as the brain (1). As an alternative, radiolabeled aa and their derivatives, such as those of phenylalanine and tyrosine, have been used by investigators to detect neoplastic tumors because these lesions show increased utilization of aa for the synthesis of proteins and other cellular components (2, 3). To accommodate the increased demand for aa, the malignant cells overexpress the aa transporters (phenylalanine and tyrosine use the L-type transporter), and this phenomenon promotes the rapid uptake and accumulation of the radiolabeled aa in the tumors. Therefore, noninvasive imaging with a radiolabeled aa can be used to detect cancerous lesions within a short time after administration of the tracer aa. Among the various radiolabeled aa tracers, [^18^F]- α-methyl-tyrosine ([^18^F]-AMT) is often used in the clinic, but the low yield of the final labeled product and the requirement of an on-site cyclotron to produce ^18^F (half-life, ~110 min) prohibit the use of this labeled compound in most oncology centers (1).

In an effort to develop an alternative to [^18^F]-AMT, Kong et al. conjugated O-[3-(1,4,8,11-tetraazabicyclohexadecane)-propyl] (N4; a metal chelator) to α-methyl tyrosine (AMT) and labeled it with ^99m^Tc ([^99m^Tc]-N4-AMT) (1). The main advantage of using ^99m^Tc instead of ^18^F is that the former nuclide has a longer half-life (~ 6 h) and can be produced in-house with a generator instead of a cyclotron. In addition, the N4 chelator in N4-AMT can also bind ^188^Re, a therapeutic nuclide that can be used to treat cancers. The biodistribution of [^99m^Tc]-N4-AMT has been investigated in normal rats, and in a separate study the labeled compound was evaluated with gamma planar imaging for the visualization of rat 13762 cell (http://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=CRL-1666&Template=cellBiology) tumors in the animals (1).

### Related Resource Links

Related chapters in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=Amino+acid+transporter+AND+micad%5Bbook%5D&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books)

Information on L-type amino acid transporters in PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=L-type%20amino%20acid%20transporter&cmd=DetailsSearch)

Inhibition of amino acid transport PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Inhibition%20of%20amino%20acid%20transport&cmd=DetailsSearch)

Nucleotide and protein (http://www.ncbi.nlm.nih.gov/nuccore?term=L-type%20amino%20acid%20transporter) sequences of mammalian amino acid transporters

L-type amino acid transporter in Online Mandelian Inheritance in Man Database (OMIM) (http://omim.org/entry/603733)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=99mTc-N4-AMT%20synthesis&cmd=DetailsSearch)]

The synthesis of N4-AMT and its labeling with ^99m^Tc have been described by Kong et al. (1). The radiochemical purity (RCP) of the labeled compound was reported to be >96% as assessed using a C18 column with reversed-phase high-performance liquid chromatography (retention time, 6.899 min). The radiochemical yield (RCY), specific activity, and stability of [^99m^Tc]-N4-AMT were not reported.

In some studies, [^99m^Tc]-N4 was used as a control, but its RCY, RCP, and specific activity were not reported (1).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=99mTc-N4-AMT%20in%20vitro%20studies&cmd=DetailsSearch)]

The uptake of [^99m^Tc]-N4-AMT and [^99m^Tc]-N4 was investigated in rat 13762 cells (1). The cells were observed to gradually accumulate radioactivity for up to 240 min only with [^99m^Tc]-N4-AMT. No such uptake by the cells was observed with [^99m^Tc]-N4. This indicated that the labeled amino acid derivative was probably taken up by the cells through the aa transport system; however, this was not confirmed with the use of appropriate aa transport inhibitors.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=99mTc-N4-AMT%20rodentia&cmd=DetailsSearch)]

The biodistribution of [^99m^Tc]-N4-AMT was investigated in normal Fischer 344 rats (n = 3 animals/time point) as described by Kong et al. (1). Each rat was injected intravenously with either 0.92 ± 0.01 MBq (25 ± 0.5 μCi) [^99m^Tc]-N4-AMT or [^99m^Tc]-N4, and the animals were euthanized at 0.5, 2, and 4 h postinjection (p.i.) to determine the amount of radioactivity accumulated in the various organs. Data obtained from this study were presented as percent of injected dose per gram tissue (% ID/g). With [^99m^Tc]-N4-AMT, maximum uptake of radioactivity was observed in the kidneys (5.77 ± 0.35% ID/g), followed by the liver (1.40 ± 0.07% ID/g) and thyroid (0.57 ± 0.04% ID/g) at 0.5 h p.i., and the label in these organs decreased to 4.74 ± 0.33% ID/g, 0.60 ± 0.02% ID/g, and 0.24 ± 0.1% ID/g, respectively, at 4 h p.i. All other organs showed an uptake between 0.03 ± 0.00% ID/g (brain) and 0.50 ± 0.02% ID/g (stomach) at 0.5 h p.i., which decreased to between 0.01 ± 0.00% ID/g (brain) and 0.43 ± 0.02% ID/g (stomach) at 4 h p.i. Data for [^99m^Tc]-N4 and blocking studies with [^99m^Tc]-N4-AMT were not reported.

In another study, Fisher 344 rats (n = 3 animals/tracer) bearing rat 13762 cell tumors on the right posterior leg were injected with either 11.11 MBq/rat (300 μCi/rat) [^99m^Tc]-N4-AMT (0.3 mg/rat) or [^99m^Tc]-N4 (0.15 mg/rat) as described above (1). Planar scintigraphic images of the animals were then acquired at 0.5, 1, and 2 h p.i. Radioactivity counts per pixel were calculated from computer-outlined regions of interest from the images of the tumors, and the normal surrounding muscle and the tumor/muscle (T/M) ratios were calculated at the different time points. The tumors were clearly visible at the various time points only in rats injected with [^99m^Tc]-N4-AMT. The T/M ratios for [^99m^Tc]-N4-AMT and [^99m^Tc]-N4 were reported to be 2.3 and 1.28, respectively, at 0.5 h p.i., and these ratios for the two tracers increased to 4 and 2.3, respectively, at 2 h p.i.

From these studies, the investigators concluded that [^99m^Tc]-N4-AMT can be used for the imaging of tumors in rodents (1).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=99mTc-N4-AMT%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=99mTc-N4-AMT%20Non-Human%20Primates&cmd=DetailsSearch)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=99mTc-N4-AMT%20Human%20Studies&cmd=DetailsSearch)]

No publication is currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## NIH Support

A part of the studies reported in this chapter were funded by a National Institutes of Health grant CA16672.

## References

1 Kong F.L., Ali M.S., Zhang Y., Oh C.S., Yu D.F., Chanda M., Yang D.J. (2011). Synthesis and evaluation of amino acid-based radiotracer 99mTc-N4-AMT for breast cancer imaging. J Biomed Biotechnol.
2 la Fougere C., Suchorska B., Bartenstein P., Kreth F.W., Tonn J.C. (2011). Molecular imaging of gliomas with PET: opportunities and limitations. Neuro Oncol.
3 Ganapathy V., Thangaraju M., Prasad P.D. (2009). Nutrient transporters in cancer: relevance to Warburg hypothesis and beyond. Pharmacol Ther.